# ^111^In/^68^Ga-Labeled DOTA-conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Asp-Phe-NH_2_ (cyclo-MG1), a minigastrin analog

Chemical name: | ^111^In/^68^Ga-Labeled DOTA-conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Asp-Phe-NH_2_ (cyclo-MG1), a minigastrin analog
Abbreviated name: | [^111^In/^68^Ga]-DOTA-cycloMG1
Synonym:
Agent Category: | Peptide
Target: | Cholecystokinin receptor subtype 2 (CCK2R)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT) and gamma planar imaging for ^111^In; positron emission tomography (PET) for ^68^Ga
Source of signal / contrast: | ^111^In (SPECT); ^68^Ga (PET)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cck2%20receptor&cmd=DetailsSearch)]

The three subtypes of the cholecystokinin (CCK) receptors (CCKR) belong to the G-protein–coupled receptor family and are classified (CCK1R, CCK2R, and CCK2i4svR) on the basis of their affinities for the CCK and the gastrin peptides, differential distribution in the tissues, and molecular structure (1). The CCK1R (previously known as CCKA) is found mainly on the peripheral cells of the pancreas and has 500- to 1,000-fold higher affinity for sulfated CCK compared with the non-sulfated ligand. In addition, the CCK1R is expressed mainly in organs of the gastrointestinal tract of rodents, while it is expressed at low levels in humans (2). The CCK2R (previously known as CCKB) is expressed in the brain, stomach, pancreas, and gallbladder and exhibits an almost equivalent affinity for gastrin and sulfated or non-sulfated CCK (the CCK2R is also known as the gastrin receptor (GR)). Although CCK1R and CCK2R/GR are expressed in various normal tissues, the CCK2R is overexpressed in most tumor tissues, such as medullary thyroid carcinomas (http://www.cancer.gov/cancertopics/pdq/genetics/medullarythyroid/HealthProfessional) (MTC; >90%), astrocytomas (http://www.cancer.gov/dictionary?cdrid=45602) (>65%), and stromal ovarian cancers (http://www.cancer.gov/cancertopics/types/ovarian) (100%). The CCK2i4svR is a splice variant of the CCK2R that is expressed only in colorectal and pancreatic neoplasms, with no expression in normal colorectal mucosa (1). Several gastrin and CCK analogs that have a high affinity for the CCK2R have been developed and labeled with radionuclides for the detection and therapy of these cancers. It has been shown that radiolabeled CCK derivatives and minigastrin (MG; a shorter version of human gastrin 1 that consists of amino acids 5–17 of the parent peptide) can be used with scintigraphy to detect colorectal or pancreatic cancer tumors that overexpress the CCK2i4svR (3) or to screen for patients who may benefit from the radiotherapy of this disease (4). In preclinical studies, however, these radiochemicals have shown a high uptake of radioactivity in the kidneys, thereby limiting their use in humans (5).

Two cyclized MG analogs, cyclo-MG1 (cyclo^1,9^[γ-D-Glu^1^,desGlu^2^−^6^,D-Lys^9^]MG) and cyclo-MG2 (cyclo^1,9^[γ-D-Glu^1^,desGlu^2^−^6^,D-Lys^9^,Nle^11^]MG) were synthesized, conjugated to metal chelating agents, labeled with ^99m^Tc through ethylenediamine-N,N-diacetic acid/hydrazinonicotinicamide (EDDA/HYNIC) bifunctional chelating agents and evaluated with single-photon emission computed tomography (SPECT) for the detection of tumors that express the CCKRs (6). The two ^99m^Tc-labeled cyclo-compounds were shown to be suitable to detect tumors, but they exhibited low in vitro stability and generated low-quality scintigraphic images due to rapid degradation in vivo. Similar observations have been reported with other ^99m^Tc-labeled compounds that were used in a clinical trial for the visualization of tumors that overexpress the CCK2R (7). In an ongoing effort to develop imaging agents that could be used to visualize tumors that express the CCK2R, two 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-conjugated cyclic MG analogs, cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Asp-Phe-NH_2_ (DOTA-cyclo-MG1) and cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Nle-Asp-Phe-NH_2_ (DOTA-cyclo-MG2), were designed for labeling with either ^111^In (for SPECT imaging) or ^68^Ga (for imaging with positron emission tomography (PET)) (5). The biodistribution of the various radiolabeled compounds and their ability to detect xenograft tumors that express the CCK2R in mice was then investigated. This chapter presents the results obtained with ^111^In/^68^Ga-labeled DOTA-cyclo-MG1 ([^111^In/^68^Ga]-DOTA-cyclo-MG1). The biodistribution and imaging characteristics of ^111^In/^68^Ga-labeled DOTA-cyclo-MG2 are presented in a companion chapter in MICAD (www.micad.nih.gov) (8).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=CCKR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Mouse cholecystokinin B receptor (CCK2R (http://www.ncbi.nlm.nih.gov/gene/12426)); NCBI-Gene ID: 12426

Mouse CCK2R nucleotide and protein (http://www.genome.jp/dbget-bin/www_bget?mmu:12426) sequences in Kyoto Encyclopedia of Genes and Genomes database (KEGG)

KEGG pathway (mouse CCK2R (http://www.genome.jp/dbget-bin/get_linkdb?-t+pathway+mmu:12426))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cholecystokinin+receptor) related to cholecystokinin receptor

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyclo-MG1%20synthesis&cmd=DetailsSearch)]

DOTA-cyclo-MG1 was obtained from a commercial source and characterized with matrix-assisted laser desorption/ionization-time of flight mass spectrometry and reverse-phase high-performance liquid chromatography (RP-HPLC) (5). The peptide was labeled with ^111^In or ^68^Ga as described by von Guggenberg et al. (5). The specific activities of the labeled peptides were 2.7–4.1 MBq/nmol (72.9–110.7 μCi/nmol) and 5.3–13.6 MBq/nmol (143.1–367.2 μCi/nmol) with ^111^In and ^68^Ga, respectively. The radiochemical purities of both peptides were >95% as determined with RP-HPLC. The radiochemical yields of the labeled peptides were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG1%20in%20vitro&cmd=DetailsSearch)]

Because ^68^Ga has a short half-life (~68 min), all the in vitro characterization studies were performed only with [^111^In]-DOTA-cyclo-MG1 (half-life of ^111^In is ~2.8 d) (5). The in vitro stability of [^111^In]-DOTA-cyclo-MG1 was determined by incubating 500–1,000 pmol of the radiochemical for up to 24 h at 37°C in phosphate-buffered saline (PBS; pH not mentioned) and fresh human plasma, respectively. Although >95% of the labeled peptide remained intact in PBS at 24 h after the incubation (as determined with RP-HPLC analysis), only 70% of the tracer was reported to be unaltered in the plasma at the end of the incubation. In another study, size-exclusion chromatographic analysis of a [^111^In]-DOTA-cyclo-MG1 and human plasma mixture incubated for 4 h at 37°C showed that only 20.4 ± 0.4% (instead of the 30% observed in the study mentioned above) of the tracer was bound to the plasma proteins (5). Radio-HPLC analysis of [^111^In]-DOTA-cyclo-MG1 (500–1,000 pmol peptide/mL) that had been incubated with rat liver and kidney homogenates for 2 h at 37°C revealed that the labeled peptide was completely degraded within this time period (5).

Using an octanol/water mixture, the partition coefficient (log P) of [^111^In]-DOTA-cyclo-MG1 was determined to be −3.08 ± 0.12.

The receptor binding and cell uptake characteristics of [^111^In]-DOTA-cyclo-MG1 were studied with AR42J cells, a rat pancreatic cell line that expresses the CCK2R (5). Incubation of the labeled peptide with the cells for 2 h showed that 1.74 ± 0.07% of the total added radioactivity was internalized by the cells. From an autoradiographic assay with human tumors known to express the CCK2R and using ^125^I-labeled CCK as the receptor ligand in the presence of DOTA-cyclo-MG1, it was determined that the IC_50_ value of the cyclic peptide for the receptor was 0.7 ± 0.12 nM (n = 3 determinations). For comparison, the IC_50_ value of CCK-8, a control linear peptide with high affinity for the CCKR, was reported to be 0.06 ± 0.04 nM in the same assay.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In/^68^Ga]-DOTA-cyclo-MG1 was investigated in BALB/c nude mice bearing AR42J cell xenograft tumors on their right flank (5). The animals (n = 3 mice/time point per tracer) were injected through the tail vein with a mixture of 0.05 MBq (1.35 μCi) [^111^In]-DOTA-cyclo-MG1 and 1 MBq (27 μCi) [^68^Ga]-DOTA-cyclo-MG1 (this corresponded to <0.12 nmol total peptide). The mice were subsequently euthanized at 1 h and 4 h postinjection (p.i.) to determine the amount of radioactivity present in the various organs. All results were expressed as percent of injected dose per gram tissue (% ID/g). Data in Table 1 shows that there were differences in the biodistribution of radioactivity from [^111^In]-DOTA-cyclo-MG1 and [^68^Ga]-DOTA-cyclo-MG1 in the tumor-bearing rodents (5). In general, the accumulation of radioactivity in the various organs and the tumors was higher with [^68^Ga]-DOTA-cyclo-MG1 than with [^111^In]-DOTA-cyclo-MG1 (Table 1). However, the tumor/muscle ratios with the two labeled compounds were quite similar (10.56 and 11.54 with [^111^In]-DOTA-cyclo-MG1 and [^68^Ga]-DOTA-cyclo-MG1, respectively). In addition, radioactivity from [^111^In]-DOTA-cyclo-MG1 was excreted primarily through the renal route, whereas radioactivity from [^68^Ga]-DOTA-cyclo-MG1 was excreted mainly through the hepatobiliary route. To determine the receptor binding specificity of the two tracers, the animals (n = 3 mice) were injected with a mixture of the two tracers along with ~30 nmol non-radioactive human MG (5). The animals were euthanized at 1 h p.i., and all tissues of interest were retrieved from the mice as before. The uptake of radioactivity in the tumors was reduced by ~50% with both the labeled compounds (Table 1), indicating that the two radiolabeled chemicals had a moderate binding specificity for the CCK2R.

For SPECT imaging studies, a mouse bearing AR42J cell tumors was injected with 10–15 MBq (27–40.5 μCi) [^111^In]-DOTA-cyclo-MG1 (~0.3 nmol peptide) as described above (5). Images acquired from the animal at 1 h p.i. showed that the tumor was visible only faintly at this time point, and the tumor/kidney ratio was calculated to be 0.01. In another study, beige SCID mice bearing A431 cell tumors transfected with the CCK2R (A431 CCK2R–positive) on the left shoulder and A431 cell tumors that did not express the CCK2R (A431 CCK2R–negative) on the right shoulder were injected with [^111^In]-DOTA-cyclo-MG1 as before (5). Whole-body SPECT/computed tomography images of the animals (n = 2 mice) showed that only the A431 CCK2R–positive tumors were visible at 1 h and 4 h p.i., and no uptake of label was apparent in the A431 CCK2R–negative lesions.

From these studies, the investigators concluded that although [^111^In]-DOTA-cyclo-MG1 appears to be suitable for use as an imaging agent to visualize tumors that express the CCK2R, further studies are necessary to improve the targeting and the metabolic and pharmacokinetic properties of this MG analog (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG1%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Laverman P., Sosabowski J.K., Boerman O.C., Oyen W.J. (2012). Radiolabelled peptides for oncological diagnosis. Eur J Nucl Med Mol Imaging.
2 Roosenburg S., Laverman P., van Delft F.L., Boerman O.C. (2011). Radiolabeled CCK/gastrin peptides for imaging and therapy of CCK2 receptor-expressing tumors. Amino Acids.
3 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
4 von Guggenberg E., Dietrich H., Skvortsova I., Gabriel M., Virgolini I.J., Decristoforo C. (2007). 99mTc-labelled HYNIC-minigastrin with reduced kidney uptake for targeting of CCK-2 receptor-positive tumours. Eur J Nucl Med Mol Imaging.
5 von Guggenberg E., Rangger C., Sosabowski J., Laverman P., Reubi J.C., Virgolini I.J., Decristoforo C. (2012). Preclinical Evaluation of Radiolabeled DOTA-Derivatized Cyclic Minigastrin Analogs for Targeting Cholecystokinin Receptor Expressing Malignancies. Mol Imaging Biol.
6 von Guggenberg E., Sallegger W., Helbok A., Ocak M., King R., Mather S.J., Decristoforo C. (2009). Cyclic minigastrin analogues for gastrin receptor scintigraphy with technetium-99m: preclinical evaluation. J Med Chem.
7 Kosowicz J., Mikolajczak R., Czepczynski R., Ziemnicka K., Gryczynska M., Sowinski J. (2007). Two peptide receptor ligands (99m)Tc-EDDA/HYNIC-Tyr(3)-octreotide and (99m)Tc-EDDA/HYNIC-(D)Glu-octagastrin for scintigraphy of medullary thyroid carcinoma. Cancer Biother Radiopharm.
8 Chopra, A., 111In/68Ga-Labeled DOTA conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Nle-Asp-Phe-NH2 (cyclo-MG2), a minigastrin analog. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.

Table 1: Accumulation of radioactivity (% ID/g) in various organs from [^111^In]-DOTA-cyclo-MG1 and [^68^Ga]-DOTA-cyclo-MG1

Tissue | [ ^ 111 ^ In]-DOTA-cyclo-MG1 | | | | [ ^ 68 ^ Ga]-DOTA-cyclo-MG1
Tissue | Time postinjection (p.i.)
Tissue | 1 h | 1 h Blocked | 4 h | Tumor/Tissue Ratio at 1 h | 1 h | 1 h Blocked | 4 h | Tumor/Tissue Ratio at 1 h
Blood | 0.35 ± 0.01 | 0.20 ± 0.02 | 0.07 ± 0.06 | 3.11 | 1.21 ± 0.04 | 0.91 ± 0.12 | 0.53 ± 0.29 | 2.47
Muscle | 0.08 ± 0.02 | 0.03 ± 0.01 | 0.01 ± 0.00 | 10.56 | 0.25 ± 0.01 | 0.23 ± 0.02 | 0.22 ± 0.10 | 11.54
Intestine | 0.31 ± 0.05 | 0.28 ± 0.05 | 0.83 ± 0.77 | 3.63 | 3.84 ± 9.15 | 2.89 ± 0.23 | 3.19 ± 0.50 | 1.41
Liver | 0.28 ± 0.06 | 0.36 ± 0.06 | 0.21 ± 0.12 | 3.23 | 1.85 ± 0.37 | 2.75 ± 0.09 | 3.10 ± 0.76 | 0.77
Kidney | 2.10 ± 0.47 | 1.67 ± 0.30 | 1.84 ± 0.37 | 0.66 | 1.48 ± 0.31 | 1.24 ± 0.20 | 1.16 ± 0.21 | 2.38
Tumor | 1.10 ± 0.20 | 0.54 ± 0.10 | 0.72 ± 0.24 | - | 3.46 ± 0.66 | 1.66 ± 0.35 | 2.94 ± 1.00 | -

For complete data, see von Guggenberg et al. ( 5 )